# ^111^In-Diethylenetriamine pentaacetic acid-bevacizumab

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-bevacizumab
Abbreviated name: | ^111^In-DTPA-bevacizumab
Synonym:
Agent category: | Antibody
Target: | Vascular endothelial growth factor (VEGF)
Target category: | Antigen
Method of detection: | SPECT, gamma planar imaging
Source of signal/contrast: | ^111^In
Activation: | No
Studies: | - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20bevacizumab)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species do (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (1).

VEGF is overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (6-8). However, several studies have shown that cancer treatments (photodynamic therapy, radiotherapy, and chemotherapy) can lead to increased tumor VEGF expression and subsequently to more aggressive disease (9, 10). Therefore, it is important to measure VEGF levels in the tumors to design better anti-cancer treatment protocols. Bevacizumab is a humanized antibody against VEGF-A (11). It binds to all VEGF isoforms. Bevacizumab is approved for clinical use in metastatic colon carcinoma and non-small cell lung cancer (12). Stollman et al. (13) prepared ^111^In-diethylenetriamine pentaacetic acid-bevacizumab (^111^In-DTPA-bevacizumab) for imaging VEGF expression in nude mice bearing LS174T human colon carcinoma xenografts.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20bevacizumab+synthesis)]

Isothiocyanate-benzyl-DTPA and bevacizumab (1:1 molar ratio) were incubated in sodium borate buffer (pH 9) for 20 h at 37°C (13). DTPA-Bevacizumab was isolated from the incubation mixture with column chromatography. DTPA-Bevacizumab (0.05 mg) in 0.15 M ammonium acetate buffer (pH 5.25) was mixed with 18.5 MBq (0.5 mCi) of ^111^InCl_3_. The mixture was incubated for 30 min at room temperature. ^111^In-DTPA-Bevacizumab was purified with column chromatography with a specific activity of 15.2 MBq/nmol (0.41 mCi/nmol) and a radiochemical purity of >97%. Nagengast et al. (14) reported a similar synthesis of ^111^In-DTPA-bevacizumab with a labeling yield of 96.6% and a specific activity of 7.6 MBq/nmol (0.2 mCi/nmol). There were two to three chelators per antibody. ^111^In-DTPA-Bevacizumab was stable for 7 d at 4°C in ammonium acetate and at 37°C in serum. ^111^In-DTPA-bevacizumab resulted in 56.9 ± 0.7% binding to immobilized VEGF. Bevacizumab and ^111^In-DTPA-bevacizumab (1:1) blocked binding by 50%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20bevacizumab+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20bevacizumab+rodentia)]

Stollman et al. (13) performed a dose escalation study of ^111^In-DTPA-bevacizumab (1, 3, 10, 30, 100, 300, and 1,000 µg/mouse) in mice bearing VEGF-expressing LS174 tumors. Muscle, tumor, and blood radioactivity levels (in percent of injected dose per gram (% ID/g)) were assessed at 3 d after injection. There were no dose-related effects in the blood (10–12% ID/g) and muscle (2–3% ID/g). On the other hand, there was an inverse correlation between antibody dose and accumulation of radioactivity in the tumor. The highest tumor accumulation (20–25% ID/g) was observed with 1 and 3 µg of ^111^In-DTPA-bevacizumab. The lowest tumor accumulation (<3% ID/g) was observed at 300 and 1,000 µg, indicating binding to a saturable site. Subsequent biodistribution studies were performed with 2 µg/mouse at 1, 3, and 6 d after injection. The organ with the highest accumulation of ^111^In-DTPA-bevacizumab was the lung (~8% ID/g) with accumulation of <3% ID/g in the liver, intestine, spleen, and kidneys at 3 d after injection. The tumor/muscle ratio was >10. Co-injection of excess bevacizumab resulted in a significant decrease in radioactivity concentration in the tumors (<3% ID/g, P < 0.005). Little inhibition was observed in the other organs. LS174 tumors, which were found to express VEGF-A mRNA, could be clearly visualized on planar scintigraphic images at 1, 3, and 7 d after injection. Nagengast et al. (14) observed a similar biodistribution pattern in mice bearing human SKOV-3 ovarian tumor xenografts with 100 ug ^111^In-DTPA-bevacizumab. The tumor accumulation was 6.17% ID/g at 3 d after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20bevacizumab+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20bevacizumab+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20bevacizumab+human)]

Scheer et al. (15) performed whole-body single-photon emission computed tomography and computed tomography scans in 12 patients with colorectal liver metastases after intravenous injection of ~200 MBq (5.4 mCi) ^111^In-bevacizumab at 10 min and 7 d after injection. Enhanced uptake of ^111^In-bevacizumab in the liver metastases was detected in 9 of the 12 patients. The level of antibody accumulation in these lesions varied considerably. There was no correlation between the level of ^111^In-bevacizumab accumulation and the level of VEGF-A expression in the tumor sections as determined with in situ hybridization and ELISA.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Gorski D.H., Beckett M.A., Jaskowiak N.T., Calvin D.P., Mauceri H.J., Salloum R.M., Seetharam S., Koons A., Hari D.M., Kufe D.W., Weichselbaum R.R. (1999). Blockage of the vascular endothelial growth factor stress response increases the antitumor effects of ionizing radiation. Cancer Res.
10 Solban N., Selbo P.K., Sinha A.K., Chang S.K., Hasan T. (2006). Mechanistic investigation and implications of photodynamic therapy induction of vascular endothelial growth factor in prostate cancer. Cancer Res.
11 Wang Y., Fei D., Vanderlaan M., Song A. (2004). Biological activity of bevacizumab, a humanized anti-VEGF antibody in vitro. Angiogenesis.
12 Ferrara N., Hillan K.J., Gerber H.P., Novotny W. (2004). Discovery and development of bevacizumab, an anti-VEGF antibody for treating cancer. Nat Rev Drug Discov.
13 Stollman T.H., Scheer M.G., Leenders W.P., Verrijp K.C., Soede A.C., Oyen W.J., Ruers T.J., Boerman O.C. (2008). Specific imaging of VEGF-A expression with radiolabeled anti-VEGF monoclonal antibody. Int J Cancer.
14 Nagengast W.B., de Vries E.G., Hospers G.A., Mulder N.H., de Jong J.R., Hollema H., Brouwers A.H., van Dongen G.A., Perk L.R., Lub-de Hooge M.N. (2007). In vivo VEGF imaging with radiolabeled bevacizumab in a human ovarian tumor xenograft. J Nucl Med.
15 Scheer M.G., Stollman T.H., Boerman O.C., Verrijp K., Sweep F.C., Leenders W.P., Ruers T.J., Oyen W.J. (2008). Imaging liver metastases of colorectal cancer patients with radiolabelled bevacizumab: Lack of correlation with VEGF-A expression. Eur J Cancer.